# (2S,3S)-2-[α-(2-[^11^C]Methylphenoxy)phenylmethyl]morpholine

Chemical name: | (2S,3S)-2-[α-(2-[^11^C]Methylphenoxy)phenylmethyl]morpholine
Abbreviated name: | [^11^C]MENET-1
Synonym: | (2S)-2-[(S)-(2-methylphenoxy)-phenylmethyl]morpholine
Agent category: | Compound
Target: | Norepinephrine transporter (NET)
Target category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+MENET)]

Many diseases affect the sympathetic nervous system (SNS), and imaging of pathological changes of adrenergic transmission has been an important area of radiopharmaceutical research (1, 2). Most postganglionic sympathetic neurons in the autonomic nervous system release the neurotransmitter norepinephrine (NE), which stimulates adrenergic receptors in various effector organs (3). There are different types and subtypes of adrenergic receptors, and they are characterized as α_1a_ to α_1c_, α_2a_ to α_2c_, and β_1_ to β_3_ (4). All of the NE adrenergic receptors belong to the G-protein–linked receptor superfamily and mediate slow neuromodulatory postsynaptic responses. The NE transporter (NET) is a transmembrane protein located in the adrenergic nerve terminals, and it is responsible for active reuptake (uptake-1) of NE released from neurons (5). NE is stored in the neuronal vesicles and is released on stimulation. Significant expression of NET is found in major organs of the SNS, such as the heart and brain. There is substantial evidence that aberrations in cardiac SNS function contribute to the morbidity and mortality associated with cardiac diseases (6). Brain NET is involved in various neurological and psychiatric diseases, including depression, attention deficit hyperactivity disorder, drug addiction, and eating disorders (7). NET is also the site of action in the brain for many antidepressant drugs (8).

Molecular probes with structures closely related to NE can be used to assess the integrity of presynaptic sympathetic nerve terminals in various diseases. In vivo NE synthesis is similar to dopamine synthesis, and dopamine is converted to NE by the enzyme dopamine-β-hydroxylase (4). [^123^I]-meta-Iodobenzylguanidine, [^11^C]meta-hydroxyephedrine, [^11^C]norepinephrine, and many other radioligands have been developed and used for peripheral neuronal imaging (9). However, this class of tracers is not suitable for the study of brain NET system because they are not able to cross the blood–brain barrier (10). In the brain, NET levels are relatively low compared with those of other transporters, such as dopamine transporter (DAT) and serotonin transporter (SERT) (8). Several NET reuptake inhibitors such as [^11^C]desipramine have been tested, but they showed high nonspecific binding. Reboxetine ((RS)-2-[((RS)-2-ethoxyphenoxy)benzyl]morpholine) is a specific NET inhibitor with a high affinity and selectivity. Reboxetine is available as a racemic mixture of the (R,R) and (S,S) enantiomers. The (S,S) enantiomer has been found to be more potent, with a 50% inhibition concentration (IC_50_) value of 3.6 nM, for inhibiting NET in rat hypothalamic synaptosomes. Among the different reboxetine derivatives that have been tested, (2S,3S)-2-[α-(2-methylphenoxy)phenylmethyl]morpholine (MENET-1) is considered a potential candidate to be developed as a radioligand for studying the brain NET system (11). ^11^C-Labeled MENET-1 ([^11^C]MENET-1) is being developed as a positron emission tomography (PET) imaging agent of NET. ^11^C is a positron emitter with a physical half-life (t_½_) of 20.4 min.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+MENET%20AND%20synthesis)]

Zeng et al. (11) reported the two-step radiosynthesis of [^11^C]MENET-1 by ^11^C methylation of the N-Boc precursor (2S,3S)-N-tert-butoxycarbonyl-2-[α-(2-trimethylstannylphenoxy)phenylmethyl]morpholine and subsequent hydrolysis to remove the N-Boc protecting group. The N-Boc precursor was reacted with [^11^C]CH_3_I for 5 min at 100ºC in the presence of Pd_2_(dba)_3_, (o-CH_3_C_6_H_4_)_3_P, CuCl, and K_2_CO_3_, followed by removal of the N-Boc group with trifluoroacetic acid (7 min at 100ºC). Radiochemical yields were 38% (decay-corrected, based on [^11^C]CH_3_I), and the synthesis time was 60 min from the end of bombardment. After purification with high-performance liquid chromatography, the final product had a radiochemical purity of >98%. The specific activity was 14.8–33.3 GBq/μmol (0.4–0.9 Ci/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+MENET%20AND%20in%20vitro)]

Zeng et al. (11) showed that binding affinities (K_i_) of MENET-1 at NET, SERT, and DAT were 1.02 ± 0.11, 93 ± 20, and 327 ± 39 nM, respectively. The binding assays were performed using HEK-293 cells transfected with the human transporters. MENET-1 exhibited a log P_7.4_ of 2.04.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+MENET%20AND%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+MENET%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+MENET%20AND%20%28primate%20NOT%20human%29)]

Zeng et al. (11) evaluated [^11^C]MENET-1 as a radioligand for PET imaging studies of brain NET in male rhesus monkeys. Imaging studies with 555–740 MBq (15–20 mCi) [^11^C]MENET-1 showed high accumulation in the thalamus, midbrain, cerebellum, and pons (NET-rich regions) and moderate accumulation in the caudate and frontal cortex. The accumulation of radioactivity in the NET-rich regions peaked between 16–28 min after injection with a clearance t_½_ from peak uptake of ~105 min. The ratios of radioactivity in the NET-rich regions to caudate were 1.30–1.45 at 45 min and remained relatively constant (1.25–1.44) at 85 min. Pretreatment with desipramine (0.25 mg/kg) 40 min before [^11^C]MENET-1 injection led to reduced radioactivity levels in the NET-rich regions, but not in the caudate or occipital cortex. The ratios of radioactivity in the NET-rich regions to caudate were reduced to 0.79–1.06 at 85 min after injection.

The norepinephrine transporter in the monkey brain was distributed heterogeneously, with highest levels occurring in the locus coeruleus complex and raphe nuclei, and moderate binding density in the hypothalamus, midline thalamic nuclei, bed nucleus of the stria terminalis, central nucleus of the amygdala, and brainstem nuclei such as the dorsal motor nucleus of the vagus and nucleus of the solitary tract. Low levels of binding to the norepinephrine transporter were measured in basolateral amygdala and cortical, hippocampal, and striatal regions. The distribution of the norepinephrine transporter in the non-human primate brain was comparable overall to that described in other species.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+MENET%20AND%20human)]

No publication is currently available.

## References

1 Konishi, J., B.A. Dwamena, M.D. Gross, B. Shapiro, T. Misaki, M. Fukunaga, J.C. Sisson, H.-Y. Oei, M. De Jong, and E. P. Krenning Endocrinology, in Molecular Nuclear Medicine, L.E. Feinendegen, W.W. Shreeve, W.C. Eckelman, Y.-W. Bahk, and H.N. Wagner Jr., Editor. 2003, Springer: New York. p. 357-409.
2 Antoni, G., T. Kihlberg, and B. Langstrom, Aspects on the synthesis of 11C-Labelled compounds, in Handbook of Radiopharmaceuticals, M.J. Welch, and C.S. Redvanly, Editor. 2003, John Wiley & Sons Ltd.: West Sussex, England. p. 141-194.
3 Sunderland, P.M., Pathophysiology. The biologic basis for disease in adults and children, K.L. McCance, and S. E. Huether, Editor. 1994, Mosby-Year Books, Inc.: St, Louiis. p. 397-436.
4 Frey, K.A., PET study of neurochemical systems, in Positron Emission Tomography, P.E. Valk, D.L. Bailey, D.W. Townsend, and M.N. Maisey, Editors. 2002, Springer London. p. 309-327.
5 Buursma A.R., Beerens A.M., de Vries E.F., van Waarde A., Rots M.G., Hospers G.A., Vaalburg W., Haisma H.J. (2005). The Human Norepinephrine Transporter in Combination with 11C-m-Hydroxyephedrine as a Reporter Gene/Reporter Probe for PET of Gene Therapy. J Nucl Med.
6 Caldwell J.H., Kroll K., Li Z., Seymour K., Link J.M., Krohn K.A. (1998). Quantitation of presynaptic cardiac sympathetic function with carbon-11-meta-hydroxyephedrine. J Nucl Med.
7 Zahniser N.R., Doolen S. (2001). Chronic and acute regulation of Na+/Cl- -dependent neurotransmitter transporters: drugs, substrates, presynaptic receptors, and signaling systems. Pharmacol Ther.
8 Wilson A.A., Johnson D.P., Mozley D., Hussey D., Ginovart N., Nobrega J., Garcia A., Meyer J., Houle S. (2003). Synthesis and in vivo evaluation of novel radiotracers for the in vivo imaging of the norepinephrine transporter. Nucl Med Biol.
9 Langer O., Halldin C. (2002). PET and SPET tracers for mapping the cardiac nervous system. Eur J Nucl Med Mol Imaging.
10 Ding Y.S., Lin K.S., Logan J., Benveniste H., Carter P. (2005). Comparative evaluation of positron emission tomography radiotracers for imaging the norepinephrine transporter: (S,S) and (R,R) enantiomers of reboxetine analogs ([11C]methylreboxetine, 3-Cl-[11C]methylreboxetine and [18F]fluororeboxetine), (R)-[11C]nisoxetine, [11C]oxaprotiline and [11C]lortalamine. J Neurochem.
11 Zeng F., Mun J., Jarkas N., Stehouwer J.S., Voll R.J., Tamagnan G.D., Howell L., Votaw J.R., Kilts C.D., Nemeroff C.B., Goodman M.M. (2009). Synthesis, radiosynthesis, and biological evaluation of carbon-11 and fluorine-18 labeled reboxetine analogues: potential positron emission tomography radioligands for in vivo imaging of the norepinephrine transporter. J Med Chem.